# [^170^Tm]-Labeled ethylenediamine tetramethylene phosphonic acid

Chemical name: | [^170^Tm]-Labeled ethylenediamine tetramethylene phosphonic acid
Abbreviated name: | [^170^Tm]-EDTMP
Synonym: | (ethylenedinitrilo)-tetramethylenephosphonic acid
Agent Category: | Compound
Target: | Bone (hydroxyapatite) at low concentration; farnesyl disphosphate (pyrophosphate) synthase (molecular target) at high concentration
Target Category: | Enzyme
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^170^Tm
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure of EDTMP for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=bone%20pain%20palliation&cmd=DetailsSearch)]

Due to the metastases of cancer in the skeletal tissue, severe bone pain affects the quality of life of most patients suffering from malignancies of the breast, prostate, lungs, thyroid, or kidneys (2, 3). Although several interventions such as analgesics, bisphosphonates, hormone therapy, and systemic radionuclide therapy are available to manage the pain, these treatments are known to have many undesirable secondary effects (3). Radiopharmaceuticals that contain nuclides, such as strontium-89 (as ^89^SrCl_2_) and samarium-153 (administered as ^153^Sm-ethylenediamine tetramethylene phosphonic acid (EDTMP)), which are commonly used for palliative care (http://www.who.int/cancer/palliative/definition/en/) of pain in the bones of these cancer patients, have been approved by the United States Food and Drug Administration (FDA) for the treatment of this condition (3). However, these are not the most ideal agents to treat pain due to bone metastases because the radionuclide either has a long half-life and generates high-energy β^–^ particles (^89^Sr has a half-life of ~50 days and E_β(max)_ = 1.49 MeV) or is short-lived and has to be produced in close vicinity to the treatment center (^153^Sm has a half-life of ~47 h, E_β(max)_ = 0.81 MeV, and Eγ = 103 keV (28%)) (2). In addition, both of these bone pain palliative agents are known to produce myelotoxicity in some patients (4). Between the two labeled compounds, ^89^SrCl_2_ appears to be the agent of choice for clinical applications because of its longer half-life, which provides the flexibility to develop a suitable treatment regimen for the patient. There is much interest to develop alternative radiolabeled compounds that do not suppress the bone marrow but are suitable to treat pain resulting from osseous metastases as discussed by Jansen et al. (4).

Recently, Das et al. evaluated the use of thulium-170 (^170^Tm has a half-life of ~128 days, E_β(max)_ = 968 keV, and Eγ = 84 keV (3.26%)) as an alternative to ^89^SrCl_2_ for the development of a bone pain palliative (2). According to these investigators, ^170^Tm would probably exhibit low myelosupression because it emits β^–^ particles of lower energy than those emitted by ^89^Sr, and the γ-photons generated by the nuclide can be used for scintigraphy to detect the accumulation and location of the radiolabel in the organs of an animal. This chapter describes the biodistribution of ^170^Tm-labeled EDTMP (^170^Tm-EDTMP) in normal Wistar rats (2).

### Other Sources of Information

Related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=Phosphonates+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

FDA approved clinical trials with EDTMP (http://clinicaltrials.gov/ct2/results?term=EDTMP), ^89^SrCl_2_ (http://clinicaltrials.gov/ct2/results?term=Strontium+chloride), and ^153^Sm (http://clinicaltrials.gov/ct2/results?term=Sm-153) complexes

Clinical trials with other bone imaging agents (http://clinicaltrials.gov/ct2/results?term=Bone+imaging)

Protein and mRNA sequence (http://www.ncbi.nlm.nih.gov/nuccore/NM_001037277.1) of human farnesyl diphosphate synthase

Gene information (http://www.ncbi.nlm.nih.gov/gene/2224) regarding human farnesyl diphosphate synthase (GeneID: 2224)

Farnesyl diphosphate synthase in Online Mendelian Inheritance in Man (OMIM) (http://www.ncbi.nlm.nih.gov/omim/134629)

Structure of farnesyl diphosphate synthase (http://www.ncbi.nlm.nih.gov/Structure/mmdb/mmdbsrv.cgi?uid=59201) complexed with a bisphosphonate

Farnesyl diphosphate synthase in Kyoto Encyclopedia of Genes and Genomes (KEGG) Pathways (http://www.genome.jp/dbget-bin/www_bget?pathway+hsa00900)

Other publications regarding EDTMP in PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=EDTMP)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=170Tm-EDTMP&cmd=DetailsSearch)]

The production of ^170^Tm and synthesis of the ^170^Tm-EDTMP complex have been described by Das et al. (2). Radiochemical yield and purity of the ^170^Tm-EDTMP complex were reported to be >99.0% as determined with paper chromatography (R_f_ of the labeled complex was 0.9–1, and that of ^170^Tm was 0) and electrophoresis (^170^Tm-EDTMP complex moved toward the anode, whereas free ^170^Tm remained at the point of application). The final formulation and specific activity of the ^170^Tm-EDTMP complex were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=170Tm-EDTMP%20in%20vitro&cmd=DetailsSearchhttp://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20in%20vitro)]

The ^170^Tm-EDTMP complex was reported to be stable for at least one month at room temperature under in vitro conditions as determined with paper chromatography and electrophoresis (2).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=170Tm-EDTMP%20rodentia&cmd=DetailsSearch)]

The biodistribution of ^170^Tm-EDTMP was studied in normal Wistar rats as described by Das et al. (2). The animals (n = 3 rats/time point, each weighing 200–250 g) were injected with ~10 MBq of the labeled complex through the lateral tail vein and euthanized at 3 h, 1 day, and 3 days postinjection (p.i.). Major organs were removed from the animals, and the amount of radioactivity accumulated in each organ/tissue was determined. At 3 h p.i., 51.65 ± 3.78% injected activity (IA)/organ was detected in the bone, and it increased to 54.56 ± 7.74% IA by 3 days p.i. Except for the gastrointestinal tract (2.41 ± 0.02% IA at 3 h p.i. and 1.05 ± 0.64% IA at 3 days p.i.) and the muscles (2.84 ± 0.32% IA at 3 h p.i. and no radioactivity detected at 3 days p.i.), all other organs accumulated between 0.02 ± 0.01% IA (spleen and heart) and 0.86 ± 0.16% IA (stomach) at 3 h p.i. and showed either no accumulation of radioactivity (spleen, lungs, heart, and blood) or a maximum of 0.36 ± 0.13% IA (kidneys) at 3 days p.i. The skeleton/blood and skeleton/muscle ratios at 3 h p.i. were 344.33 and 18.32, respectively; these ratios could not be calculated at 3 days p.i. because the blood and muscles had no accumulated radioactivity at this time point.

In another study, anesthetized normal rats (number not reported) were injected with ~20 MBq of the radiotracer as described above, and serial scintigraphic images of the animals were recorded with a gamma camera at predetermined time points (2). The complete skeleton of the animal was clearly visible at 30 min p.i., and some organs showed minor accumulation of radioactivity at this time point. By 3 h p.i., only the skeleton was observed to retain the label, and it was visible up to 60 days p.i. (the last time point).

From these studies, the investigators concluded that ^170^Tm-EDTMP accumulated selectively in the rat skeleton, and, after further investigation, this radiolabel can be developed as a potential bone pain palliative agent (2).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=170Tm-EDTMP%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=170Tm-EDTMP%20Non-Human%20Primates&cmd=DetailsSearch)]

No publications are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=170Tm-EDTMP%20Human%20Studies&cmd=DetailsSearch)]

No publications are currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Slavicek J.M., Hayes-Plazolles N. (2003). The Lymantria dispar nucleopolyhedrovirus contains the capsid-associated p24 protein gene. Virus Genes.
2 Das T., et al. (2009). (170)Tm-EDTMP: a potential cost-effective alternative to (89)SrCl(2) for bone pain palliation. Nucl Med Biol.
3 Paes F.M., Serafini A.N. (2010). Systemic metabolic radiopharmaceutical therapy in the treatment of metastatic bone pain. Semin Nucl Med.
4 Jansen D.R., et al. (2010). Targeted radiotherapy of bone malignancies. Curr Drug Discov Technol.